# Annexin V-cross-linked iron oxide-Cy5.5

Chemical name: | Annexin V-cross-linked iron oxide-Cy5.5
Abbreviated name: | AnxCLIO-Cy5.5
Synonym: | Annexin V-CLIO-Cy5.5
Agent Category: | Protein
Target: | Phosphatidylserine
Target Category: | Binding
Method of detection: | Magnetic resonance imaging (MRI), optical (near-infrared (NIR) fluorescence)
Source of signal\contrast: | Iron oxide, Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=468888), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about annexin V.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20CLIO%20and%20cy5)]

Optical fluorescence imaging is increasingly being used to obtain images of biological functions of specific targets in vitro and in small animals (1, 2). Near-infrared (NIR) fluorescence (700–900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in vitro and in small animals.

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (3). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal.

A multimodal nanoparticle probe that consists of a contrast agent and a NIR fluorochrome may provide consistent information. CLIO nanoparticles can be internalized by cells of the reticuloendothelial system and have long circulating times within an animal body. The blood half-life of CLIO is about 10 h in mice (4). The accumulation of nanoparticles in cells causes a reduction in signal intensity with T2-weighted (T2*W) spin-echo pulse sequences. NIR fluorochromes (e.g., Cy5.5) provide an improved optical (NIR) signal from tissue. CLIO-Cy5.5 has been developed as a multimodal probe for imaging.

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells like epithelial cells and immune cells (5). During apoptosis, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. PS is also accessible for annexin V binding in necrosis because of disruption of the plasma membrane. Annexin V binds to PS with high affinity (K_d_ = 7 nM). Annexin V has been radiolabeled with ^123^I, ^124^I, and ^99m^Tc for single photon emission computed tomography (SPECT) imaging (6-8). Recently, annexin V was successfully labeled with ^18^F (9, 10). ^18^F-labeled annexin V is being developed as a positron emission tomography (PET) agent for imaging apoptosis as well as necrosis. Cy5.5-Annexin V has been evaluated as an optical probe in small animals. Annexin V-CLIO-Cy5.5 (AnxCLIO-Cy5.5) is a multimodal agent that consists of CLIO nanoparticles with attachment of annexin V and Cy5.5.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20CLIO%20cy5%20and%20synthesis)]

The synthesis of AnxCLIO-Cy5.5 was described by Schellenberger et al. (11). The amino-CLIO was labeled with Cy5.5 using monofunctional N-hydroxysuccinimide ester and activated with N-succinimidyl 3-(2-pyridyldithio)propionate (SPDP) to yield 2-pyridyl disulfide-CLIO-Cy5.5 (2PySS-CLIO-Cy5.5). 2PySS-CLIO-Cy5.5 was purified by column chromatography. Annexin V was conjugated with N-succinimidyl 3-(2-pyridylthio)propionate-S-acetylthioacetate (SATA), and unreacted SATA was separated from annexin V by spin separation. SATAylated annexin V (one SATA molecule per annexin V) was reacted with 2PySS-CLIO-Cy5.5 to yield the multimodal AnxCLIO-Cy5.5, which had 3.5 annexin V molecules and 1.8 Cy5.5 molecules per nanoparticle as determined spectrophotometrically and from the concentrations of iron by assuming 2064 iron atoms per nanoparticle. AnxCLIO-Cy5.5 had a diameter of 50 nm as determined by light scattering with R1 and R2 values of 19 and 48 mM^-1^ s^-1^, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20CLIO%20cy5%20and%20in%20vitro)]

Schellenberger et al. (11) performed cell-binding assays with AnxCLIO-Cy5.5 and fluorescein isothiocyanate (FITC)-annexin V using human Jurkat T cells. AnxCLIO-Cy5.5 and FITC-annexin V bound in a similar manner to individual cells with populations of normal (2.3%) or apoptotic (camptothecin-treated) cells (29.8%). Binding of AnxCLIO-Cy5.5 to apoptotic cells had an EC_50_ of 3.7 nM. However, the AnxCLIO-Cy5.5 nanoparticle and annexin V protein may interact with the phosphatidylserine in a somewhat different fashion because of their differing abilities to inhibit FITC-annexin V (AnxCLIO-Cy5.5 IC_50_ = 39 nM; Cy5.5-annexin V IC_50_ = 7.8 nM; annexin V IC_50_ = 2.4 nM). A high NIR fluorescence signal intensity was observed with apoptotic but not with normal cells, and a corresponding decrease in MRI signal intensity of cells was obtained with a T2*W MRI image (T2*W values were 76 ms for the control and 37 ms for the apoptotic cells).

Sosnovik et al. (12) showed that the FITC-annexin V and AnxCLIO-Cy5.5 (1–10 μg Fe/ml) probes exhibited a high degree of colocalization on apoptotic neonatal cardiomyocytes (induced by cycloheximide) by fluorescence microscopy, indicating that AnxCLIO-Cy5.5 behaved similarly to FITC-annexin V. NIR imaging of the agar phantom revealed a progressive increase in fluorescence intensity as the percentage of apoptotic cardiomyocytes increased. A corresponding decrease in signal intensity was observed on the T2*W MRI images, as the percentage of apoptotic cells increased. The average relaxation rates (per second) of the various cardiomyocyte populations in the phantom were 5.3 ± 0.2, 6.9 ± 0.5, 9.1 ± 0.3, and 12.9 ± 0.4 for the 0, 3, 8, and 18% apoptotic populations, respectively. Specific uptake of control probe (CLIO-Cy5.5) by the apoptotic neonatal cardiomyocytes was not observed after 24-h exposure of up to 10 μg Fe/ml of CLIO-Cy5.5.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20CLIO%20cy5%20and%20rodentia)]

Sosnovik et al. (12) performed in vivo cardiac MRI in nine C57BL/6 mice subjected to transient (30 min) ligation of the left anterior descending coronary artery, resulting in apoptosis of up to 20% of the cardiomyocytes in the distribution of the transiently occluded coronary artery. Significant decreases in MRI signal intensity were seen on the T2*W turbo-fast low-angle shot (FLASH) images in the mice given AnxCLIO-Cy5.5 (2 mg Fe/kg) but not in mice given the control probe CLIO-Cy5.5 (2 mg Fe/kg). Myocardial T2*W was significantly lower in the mice given AnxCLIO-Cy5.5 than in the mice given CLIO-Cy5.5 (8.1 versus 13.2 ms, P < 0.01). Ex vivo fluorescence measurements of excised hearts revealed target area to background ratio was significantly higher (2.1 versus 1.1, P < 0.01).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20CLIO%20cy5%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20CLIO%20cy5%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20CLIO%20cy5%20and%20human)]

No publication is currently available.

## NIH Support

RO1CA86782, P50CA86355, R24 CA92782, CA91807

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
4 Wunderbaldinger P., Josephson L., Bremer C., Moore A., Weissleder R. (2002). Detection of lymph node metastases by contrast-enhanced MRI in an experimental model. Magn Reson Med.
5 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
6 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
7 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
8 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
9 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
10 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
11 Schellenberger E.A., Sosnovik D., Weissleder R., Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
12 Sosnovik D.E., Schellenberger E.A., Nahrendorf M., Novikov M.S., Matsui T., Dai G., Reynolds F., Grazette L., Rosenzweig A., Weissleder R., Josephson L. (2005). Magnetic resonance imaging of cardiomyocyte apoptosis with a novel magneto-optical nanoparticle. Magn Reson Med.